# 2-[^18^F]Fluoroacetate

Chemical name: | 2-[^18^F]Fluoroacetate
Abbreviated name: | [^18^F]FAC
Synonym: | 2-[^18^F]Fluoroacetic acid
Agent Category: | Compound
Target: | TCA cycle, acetyl-CoA synthetase
Target Category: | Trapped as [^18^F]fluorocitrate
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - Rodents; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20Fluoroacetate)]

Acetate is readily taken up by cells and is activated to acetyl-CoA in both the cytosol and mitochondria by acetyl-CoA synthetase. Acetyl-CoA is a common metabolic intermediate for synthesis of cholesterol and fatty acids, which are then incorporated into membrane (1). Acetyl-CoA is also oxidized in mitochondria by the tricarboxylic acid (TCA) cycle to CO_2_ and water. Some of the acetate is converted to amino acids. In normal myocardium, acetate is metabolized to CO_2_via the TCA cycle as the dominant pathway. In contrast, tumor cells convert most of the acetate into fatty acids by a key enzyme fatty acid synthetase, which is overexpressed in cancer cells (2). Acetate is predominantly incorporated into intracellular phosphatidylcholine membrane microdomains that are important for tumor growth and metastasis (3).

[^11^C]Acetate ([^11^C]ACE) has been used as a positron emission tomography (PET) tracer for studying myocardial oxidative metabolism and regional myocardial blood flow (4) and for imaging renal, pancreatic, and prostate tumors (5). However, the potential for widespread use of [^11^C]ACE is limited by the short half-life of ^11^C (20 min). Fluoroacetate, an analog of acetate (6), is metabolized to fluoroacetyl-CoA and then fluorocitrate, which cannot be further metabolized to CO_2_ and water (7). Therefore, fluorocitrate is trapped in the cell in proportion to oxidative metabolism. [^18^F]Fluoroacetate ([^18^F]FAC) is being evaluated as a PET agent for imaging prostate cancer.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20Fluoroacetate%20and%20synthesis)]

Synthesis of [^18^F]FAC was reported by several groups with a long synthesis time (>60 min) and a low radiochemical yield (<34%) (8, 9). Sun et al. (10) and Ponde et al. (11) recently reported an automated synthesis of [^18^F]FAC with a commercial 2-[^18^F]fluoro-2-deoxy-2-D-glucose ([^18^F]FDG) synthesizer. [^18^F]FAC was prepared by nucleophilic substitution of ethyl-O-mesyl-glycolate with K[^18^F]F/Kryptofix 2.2.2 for 5 min at 100–105°C to form ethyl-[^18^F]FAC, which was hydrolyzed by NaOH to form [^18^F]FAC. This method produced [^18^F]FAC with radiochemical yields of 55 ± 5% in 35 min and radiochemical purity of >99%, decay-corrected to the end of bombardment. The average specific activity of [^18^F]FAC was 74–130 GBq/µmol (2.0–3.5 Ci/µmol) at the end of synthesis.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20Fluoroacetate%20and%20in%20vitro)]

No publication is currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20Fluoroacetate%20and%20rodentia)]

Ponde et al. (11) performed a biodistribution study in mature male rats (n = 5 per group) with [^11^C]ACE at 20 and 60 min after injection and with [^18^F]FAC at 20, 60, 120, and 240 min after injection. Biodistribution data of [^11^C]ACE showed a rapid clearance (30–60%) at 60 min from most of the organs studied. However, radioactivity from the pancreas did not clear after 60 min. [^18^F]FAC cleared significantly more slowly from the organs investigated, including the pancreas (P < 0.001). After injection of [^18^F]FAC, the radioactivity in bone increased significantly over time (P < 0.001), which suggests defluorination. There was no significant difference in uptake in the normal prostate between [^18^F]FAC and [^11^C]ACE at 60 min (0.28 ± 0.05% injected dose/g (ID/g) vs. 0.28 ± 0.04% ID/g, respectively). There was a slight but significant decrease in [^18^F]FAC uptake in the normal prostate over time (0.30 ± 0.05% ID/g at 20 min, 0.28 ± 0.05% ID/g at 1 h, 0.23 ± 0.01% ID/g at 2 h, and 0.20 ± 0.03% ID/g at 4 h; P = 0.002).

Ponde et al. (11) also a performed biodistribution study in 4- to 6-week-old nude mice bearing CWR22 human prostate carcinoma xenografts (n = 4 per group) with [^11^C]ACE at 30 min after injection and with [^18^F]FAC at 30 and 120 min after injection. The uptake in normal prostate at 30 min was significantly higher for [^18^F]FAC compared with [^11^C]ACE (2.60 ± 0.50% ID/g vs. 0.60 ± 0.17% ID/g, respectively; P < 0.001). In contrast, [^18^F]FAC uptake in the tumor at 30 min was ~4 times higher than [^11^C]ACE uptake at 30 min (4.01 ± 0.32% ID/g vs. 0.78 ± 0.06% ID/g, respectively; P < 0.001). The uptake of [^18^F]FAC was significantly higher than the uptake of [^11^C]ACE in all organs studied with exception of the spleen. There was also a notable increase of radioactivity in the bone from 30 min to 120 min. On the basis of [^18^F]FAC microPET imaging data obtained at 30, 60, and 120 min after injection, the tumor was clearly delineated in the mice (n = 2) with tumor/muscle ratios of 1.40–1.44.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20Fluoroacetate%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20Fluoroacetate%20and%20%28primate%20not%20human%29)]

Ponde et al. (11) reported that there was no extensive defluorination in a PET study with one male baboon, as indicated by [^18^F]FAC standardized uptake values (SUVs): SUVs of iliac bones and femurs were 0.26 and 0.3 at 60 min and 0.22 and 0.4 at 120 min, respectively). The organs with greatest uptake were the kidneys and liver with SUVs of 3.7 and 1.3, respectively. The brain and muscle exhibited SUVs <1.0. Further evaluation of [^18^F]FAC as a prostate cancer imaging agent and its mechanism of action are needed.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20Fluoroacetate%20and%20human)]

No publication is currently available.

## NIH Support

HL27970, NS15654, NS20867, NH37916, CA83060

## References

1 Howard B.V., Howard W.J. (1975). Lipids in normal and tumor cells in culture. Prog Biochem Pharmacol.
2 Swinnen J.V., Heemers H., Deboel L., Foufelle F., Heyns W., Verhoeven G. (2000). Stimulation of tumor-associated fatty acid synthase expression by growth factor activation of the sterol regulatory element-binding protein pathway. Oncogene.
3 Swinnen J.V., Van Veldhoven P.P., Timmermans L., De Schrijver E., Brusselmans K., Vanderhoydonc F., Van de Sande T., Heemers H., Heyns W., Verhoeven G. (2003). Fatty acid synthase drives the synthesis of phospholipids partitioning into detergent-resistant membrane microdomains. Biochem Biophys Res Commun.
4 Visser F.C. (2001). Imaging of cardiac metabolism using radiolabelled glucose, fatty acids and acetate. Coron Artery Dis.
5 Schoder H., Larson S.M. (2004). Positron emission tomography for prostate, bladder, and renal cancer. Semin Nucl Med.
6 Patel S.S., Walt D.R. (1987). Substrate specificity of acetyl coenzyme A synthetase. J Biol Chem.
7 Clarke D.D. (1991). Fluoroacetate and fluorocitrate: mechanism of action. Neurochem Res.
8 Bosch A.L., Degrado T.R., Gatley S.J. (1986). Preparation of no carrier added fluorine-18 labeled 16-fluorohexadecanoic and fluoroacetic acids from highly reactive tetraethylammonium [18F]fluoride. Int J Rad Appl Instrum [A].
9 Sykes T.R., Ruth T.J., Adam M.J. (1986). Synthesis and murine tissue uptake of sodium [18F]fluoroacetate. Int J Rad Appl Instrum B.
10 Sun L.Q., Mori T., Dence C.S., Ponde D.E., Welch M.J., Furukawa T., Yonekura Y., Fujibayashi Y. (2006). New approach to fully automated synthesis of sodium [18F]fluoroacetate -- a simple and fast method using a commercial synthesizer. Nucl Med Biol.
11 Ponde D.E., Dence C.S., Oyama N., Kim J., Tai Y.C., Laforest R., Siegel B.A., Welch M.J. (2007). 18F-Fluoroacetate: A Potential Acetate Analog for Prostate Tumor Imaging--In Vivo Evaluation of 18F-Fluoroacetate Versus 11C-Acetate. J Nucl Med.